# Cy5.5-Conjugated matrix metalloproteinase cleavable peptide nanoprobe

Chemical name: | Cy5.5-Conjugated matrix metalloproteinase cleavable peptide nanoprobe
Abbreviated name: | Cy5.5-MMP probe
Synonym:
Agent Category: | Peptide
Target: | Matrix metalloproteinase
Target Category: | Enzyme
Method of detection: | Optical imaging (near-infrared fluorescence (NIRF) imaging)
Source of signal / contrast: | Cy5.5
Activation: | Yes
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=mmp%20review&cmd=DetailsSearch)]

Matrix metalloproteinases (MMPs) are zinc-dependent endopeptidase enzymes that are known to regulate diverse physiological processes such as cell growth, differentiation, and migration, and they play an important role in the development and progression of osteoarthritis (1) and cancer (2, 3). The classification, structural characteristics, induction, regulation, and biological functions of >25 MMPs have been reviewed by Klein and Bischoff (3). Because MMPs are overexpressed in malignant tumors and support the establishment of neoplasms, these enzymes are the target of many anti-cancer drugs (4). In addition, researchers are interested to develop and evaluate imaging probes that target the MMPs so as to detect cancers at an early stage, track progression of the disease, and monitor the response to cancer therapy (5). A strategy using activatable cell-penetrating peptides (ACPPs) labeled with a radionuclide (6) or an optical imaging dye (7) has been utilized by investigators for the successful detection of tumors that overexpress MMPs in mice. However, it was shown that the ACPP probe was probably not suitable for the detection of these lesions because the probe was most likely activated in the vasculature and the tumors showed nonspecific uptake of the label (6).

Investigators have used fluorogenic probes that consist of a fluorophore and a quencher attached to a targeting peptide for in vivo detection of the MMP activity (1). A characteristic feature of these probes is that, in the normal state, fluorescence emitted by the fluorophore is absorbed by the quencher through resonance energy transfer and no signal is detected from the peptide (for a schematic diagram, see Ryu et al. (1)). The fluorescence generated by the probe is detectable only when the targeting peptide is cleaved by a suitable protease such as the MMP and the quencher is released from the complex. A limitation of using these probes in vivo is that they exhibit low stability and the constituent peptides may be cleaved nonspecifically by different proteases (1). Therefore, it was apparent that a probe containing a substrate peptide that is specific for an MMP would be most suitable for the detection of these enzymes. On the basis of this information, a fluorogenic probe containing an MMP-13–specific peptide substrate (Gly-Pro-Leu--Gly-Met-Arg-Gly-Leu-Gly-Lys; the substrate amino acid sequence is italicized, and the MMP cleavage site is indicated with a double hyphen) sandwiched between the Cy5.5 fluorescence dye and the black hole quencher-3 (BHQ-3) (http://www.biosearchtech.com/support/applications/dyes-from-biosearch-technologies/black-hole-quencher%C2%AE-dyes) was developed (1). The intact probe (Cy5.5-MMP probe) exhibited low background fluorescence that increased significantly only after the peptide substrate was cleaved by the MMP. The biodistribution of the Cy5.5-MMP probe and its ability to detect neoplastic lesions in mice bearing murine squamous cell carcinoma SCC-7 cell tumors were investigated by Yhee et al. (8).

### Related Resource Links

MMP-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books?term=MMP%20AND%20micad%5Bbook%5D&cmd=DetailsSearch)

Human MMP-13 protein and mRNA sequences (http://www.ncbi.nlm.nih.gov/nuccore/NM_002427.3)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=MMP) related to MMPs

MMP in Online Mendelian Inheritance in Man database (http://www.ncbi.nlm.nih.gov/omim?term=Matrix%20metalloproteinase) (OMIM)

Osteoarthritis-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books?term=Osteoarthritis%20AND%20micad%5Bbook%5D&cmd=DetailsSearch)

What is osteoarthritis? PubMed Health (http://www.ncbi.nlm.nih.gov/pubmedhealth/PMH0001460/)

Osteoarthritis related clinical trials (http://clinicaltrials.gov/ct2/results?term=Osteoarthritis)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Cy5.5-MMP%20synthesis&cmd=DetailsSearch)]

The MMP substrate peptide was synthesized with standard solid-phase Fmoc chemistry, and the Cy5.5-MMP probe was prepared as described by Ryu et al. (1). The final Cy5.5-labeled probe was characterized with ultraviolet-visible spectroscopy and matrix-assisted laser desorption/ionization-time of flight mass spectroscopy. Purity of the final preparation of Cy5.5-MMP was reported to be >95% as determined with reverse-phase high-performance liquid chromatography (8). The formulation, stability, storage conditions, and the ratio of Cy5.5 to the MMP peptide in the probe were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Cy5.5-MMP%20in%20vitro&cmd=DetailsSearch)]

Generation of fluorescence by Cy5.5-MMP was investigated by incubating 20 nM of the probe with increasing concentrations of MMP-13 (2 nM, 4 nM, and 8 nM) in a 96-well microplate for 30 min at 37°C as described by Yhee et al. (8). Control wells either contained no MMP-13 or had the protease in the presence of an inhibitor (4 nM; the nature of the inhibitor was not reported). Measurement of the fluorescence intensity of the wells showed that wells with 2 nM, 4 nM, and 8 nM of the protease had 13.4-, 24.7-, and 48.4-fold higher fluorescence intensity, respectively, compared with the wells without any MMP-13 or with the protease inhibitor. This indicated that the MMP probe was functional.

To confirm that the Cy5.5-MMP probe is suitable for in vitro detection of the MMP activity, different concentrations of the fluorescence-labeled peptide (ranging from 3.125 nM to 50 nM) were incubated as before with serum-free growth medium harvested from SCC-7 cells (these cells express and secrete the MMP into the growth medium) in a 96-well microplate (8). For use as controls, similar concentrations of the probe were exposed to distilled water. Fluorescence imaging of the plates showed that approximately 400 units, 600 units, and 900 units of fluorescence were generated with 12.5 nM, 25 nM, and 50 nM of the probe, respectively. The control wells exhibited constant fluorescence intensity at all concentrations of the optical probe (approximately 200 units).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Cy5.5-MMP%20rodentia&cmd=DetailsSearch)]

Biodistribution of the Cy5.5-MMP probe was investigated in nude mice bearing SCC-7 cell tumors (8). The animals (n = 5 mice/group) were injected with 40 nM of the probe through the tail vein, and fluorescence images were acquired from the animals at different time periods from 1 h to 12 h postinjection (p.i.). At 1 h p.i. the tumor was visible in the images, and the fluorescence intensity from the lesion peaked at approximately 6.25 × 10^4^ counts/sec at 3 h p.i. By 12 h p.i., the intensity decreased to approximately 4.75 × 10^4^ counts/sec. Ex vivo fluorescence imaging of various organs obtained from the animals at 3 h p.i. showed that maximum fluorescence intensity was generated in the tumors (approximately 200 counts/sec), followed by the kidneys (approximately 75 counts/sec) and the liver (approximately 50 counts/sec). Fluorescence microscopy and immunostaining of the tumor and liver tissues showed that the protease activity was present mainly in the tumor tissue and only low levels of enzyme activity were evident in the liver. No blocking studies were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Cy5.5-MMP%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Cy5.5-MMP%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Cy5.5-MMP%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Ryu J.H., Lee A., Na J.H., Lee S., Ahn H.J., Park J.W., Ahn C.H., Kim B.S., Kwon I.C., Choi K., Youn I., Kim K. (2011). Optimization of matrix metalloproteinase fluorogenic probes for osteoarthritis imaging. Amino Acids.
2 Hua H., Li M., Luo T., Yin Y., Jiang Y. (2011). Matrix metalloproteinases in tumorigenesis: an evolving paradigm. Cell Mol Life Sci.
3 Klein T., Bischoff R. (2011). Physiology and pathophysiology of matrix metalloproteases. Amino Acids.
4 Gialeli C., Theocharis A.D., Karamanos N.K. (2011). Roles of matrix metalloproteinases in cancer progression and their pharmacological targeting. FEBS J.
5 Scherer R.L., McIntyre J.O., Matrisian L.M. (2008). Imaging matrix metalloproteinases in cancer. Cancer Metastasis Rev.
6 van Duijnhoven S.M.J., Robillard M.S., Nicolay K., Grull H. (2011). Tumor Targeting of MMP-2/9 Activatable Cell-Penetrating Imaging Probes Is Caused by Tumor-Independent Activation. Journal of Nuclear Medicine.
7 Olson E.S., Jiang T., Aguilera T.A., Nguyen Q.T., Ellies L.G., Scadeng M., Tsien R.Y. (2010). Activatable cell penetrating peptides linked to nanoparticles as dual probes for in vivo fluorescence and MR imaging of proteases. Proc Natl Acad Sci U S A.
8 Yhee J.Y., Kim S.A., Koo H., Son S., Ryu J.H., Youn I.C., Choi K., Kwon I.C., Kim K. (2012). Optical imaging of cancer-related proteases using near-infrared fluorescence matrix metalloproteinase-sensitive and cathepsin B-sensitive probes. Theranostics.